# ^99m^Tc-Interleukin-18-binding protein-Fc-interlukin-1 receptor antagonist

Chemical name: | ^99m^Tc-Interleukin-18-binding protein-Fc-interlukin-1 receptor antagonist
Abbreviated name: | ^99m^Tc-IL-18bp-Fc-IL-1ra
Synonym:
Agent category: | Polypeptide
Target: | Interleukin-18 (IL-18) and IL-1 receptors
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=89111129), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_173042.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=10068) for more information about the IL-18bp.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp-Fc-IL-1ra)]

Interleukin-18 (IL-18) is a proinflammatory cytokine produced by macrophages, epithelial cells, and activated T cells (1, 2), and it plays an important role in inflammation and immune response (3, 4). IL-18 induces production of tumor necrosis factor and IL-1 in mononuclear cells. A variety of normal and malignant cells can produce and respond to IL-18 through its receptor (IL-18R). A soluble secreted IL-18 binding protein (IL-18bp) was found to bind to IL-18 with high affinity (dissociation constant (K_d_) = 0.4 nM) and to neutralize the biological effects of IL-18 by blocking its interaction with IL-18R (5, 6). IL-18bp-Fc is a 40-kDa glycoprotein with an immunoglobulin (Ig) domain.

The interleukin-1 family of two proinflammatory cytokines, IL-1α and IL-1β, which bind to two IL-1 receptors (IL-1R1 and IL-1R2), and an IL-1R antagonist (IL-1ra), is mainly produced by activated macrophages and tissue macrophages (7). IL-1α and IL-1β are important mediators of the inflammatory response and hematopoiesis, and they are involved in a variety of cellular activities, including cell proliferation, differentiation, and apoptosis. IL-1 is involved in chronic inflammatory diseases and in neuropathological conditions (8, 9). The balancing action of IL-1 and IL-1ra plays an important role in the regulation of inflammation and immune responses (10). IL-1ra has been shown to be effective as an anti-inflammatory treatment in several chronic inflammatory diseases and stroke (11, 12). A human recombinant, non-glycosylated form of the human IL-1ra (rhIL-1ra, Anakinra (http://google2.fda.gov/search?q=anakinra&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1&requiredfields=-archive%3AYes)) has been approved by the United States Food and Drug Administration for the treatment of rheumatoid arthritis (13).

IL-1 and IL-18 exhibit additive or synergistic effects in promoting pathophysiological processes observed in many inflammatory diseases (14). A dual domain IL-18bp-Fc-IL-1ra fusion protein was constructed by joining IL-18bp and IL-1ra cDNA to the Fc fragment of human IgG_1_ cDNA in an expression plasmid (15). The amino-terminal segment binds to IL-18, and the carboxyl-terminal sequence binds to the IL-1R. Liu et al. (15) radiolabeled IL-18bp-Fc-IL-1ra with ^99m^Tc via 2-iminothiolane reduction to produce ^99m^Tc-IL-18bp-Fc-IL-1ra for use with single-photon emission computed tomography (SPECT) imaging of inflammation in mice.

### Related Resource Links:

- Chapters in MICAD (IL-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=IL-1%20%5BAll+Fields%5D+AND+micad%5Bbook%5D), IL-18 (http://www.ncbi.nlm.nih.gov/books/?term=IL-18+%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (IL-1á (http://www.ncbi.nlm.nih.gov/gene/3552), IL-1â (http://www.ncbi.nlm.nih.gov/gene/3553), IL-1R1 (http://www.ncbi.nlm.nih.gov/gene/3554), IL-1R2 (http://www.ncbi.nlm.nih.gov/gene/7850), IL-1ra (http://www.ncbi.nlm.nih.gov/gene/3557), IL-18 (http://www.ncbi.nlm.nih.gov/gene/3606), IL-18R (http://www.ncbi.nlm.nih.gov/gene/8809))
- Articles in Online Mendelian Inheritance in Man (OMIM) (IL-1á (http://omim.org/entry/147760), IL-1â (http://omim.org/entry/147720), IL-1R1 (http://omim.org/entry/147810), IL-1R2 (http://omim.org/entry/147811), IL-1ra (http://omim.org/entry/147679), IL-18 (http://omim.org/entry/600953), IL-18R (http://omim.org/entry/604494))
- Clinical trials (IL-1 (http://www.clinicaltrials.gov/ct2/results?term=IL-1&Search=Search), IL-1ra (http://www.clinicaltrials.gov/ct2/results?term=il-1ra&Search=Search), Anakinra (http://www.clinicaltrials.gov/ct2/results?term=anakinra), IL-18 (http://www.clinicaltrials.gov/ct2/results?term=IL-18&Search=Search))
- Drug information in FDA (Anakinra (http://google2.fda.gov/search?q=anakinra&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1&requiredfields=-archive%3AYes))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp-Fc-IL-1ra+and+synthesis)]

Liu et al. (15) reported the synthesis of ^99m^Tc-IL-18bp-Fc-IL-1ra. IL-18bp-Fc-IL-1ra was incubated with 2-iminothiolane for 30 min at 37°C in phosphate-buffered saline (PBS, pH 7.4). A solution of 1,110 MBq (30 mCi) ^99m^TcO_4_− was added to a mixture of SnCl_2_ and glucoheptonic acid and incubated at room temperature for 5 min to produce ^99m^Tc-glucoheptonate, which was then incubated with the thiolated IL-18bp-Fc-IL-1ra for 30 min at room temperature, with a radiolabel yield of 75%. ^99m^Tc-IL-18bp-Fc-IL-1ra was purified on a PD-10 column, with >95% radiochemical purity. The specific activity was 7.4–8.3 MBq/µg (0.20–0.22 mCi/µg). ^99m^Tc-IL-18bp-Fc-IL-1ra remained >95% intact for up to 5 h in both saline at room temperature and serum at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp-Fc-IL-1ra+AND+in+vitro)]

Liu et al. (15) performed binding competition experiments with ^99m^Tc-IL-18bp-Fc-IL-1ra (2 nM) and IL-18bp-Fc-IL-1ra (0.1–10,000 nM) using rat leukocytes, which contain both IL-18R and IL-1R. The IC_50_ value for IL-18bp-Fc-IL-1ra was 73.56 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp-Fc-IL-1ra+AND+rodentia)]

Liu et al. (15) performed ex vivo biodistribution studies in normal mice and mice with TPA-induced edema in the right ears (n = 3–5/group) at 3 h after intravenous injection of 74 MBq (2 mCi) ^99m^Tc-IL-18bp-Fc-IL-1ra. The biodistribution pattern was similar for the TPA-treated mice and the normal mice, with the highest accumulation in the liver (23% injected dose/gram (ID/g), followed by the intestine (15% ID/g), kidneys (10% ID/g), spleen (3.6% ID/g), blood (1.1% ID/g), lung (0.8% ID/g), and stomach (0.7% ID/g). Low radioactivity levels (<0.4% ID/g) were found in the heart, skin, and muscle. In the TPA-treated mice, the inflamed right ears accumulated 1.80 ± 0.17% ID/g versus 0.48 ± 0.07% ID/g (P < 0.01) in the contralateral left ears. Pretreatment with excess unlabeled IL-18bp-Fc-IL-1ra 30 min before the tracer reduced the radioactivity levels to 1.09 ± 0.08% ID/g (right ears) versus 0.53 ± 0.13% ID/g (left ears) (P < 0.05). The levels of IL-1β and IL-18 were significantly increased in the TPA-treated ears compared with contralateral ears (IL-1β: 3,987 ± 40 pg/ml versus 556 ± 196 pg/ml, P < 0.01; IL-18: 223 ± 19 pg/ml versus 139 ± 12 pg/ml, P < 0.05). SPECT imaging at 3 h showed that the TPA-treated ears were clearly visualized, whereas the contralateral ears were almost invisible. Pretreatment with excess unlabeled IL-18bp-Fc-IL-1ra markedly reduced the radioactivity in the TPA-treated ears.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp-Fc-IL-1ra+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp-Fc-IL-1ra+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp-Fc-IL-1ra+AND+human)]

No publication is currently available.

## NIH Support

R01 HL090716, P41 EB002035

## References

1 Dinarello C.A. (1999). Interleukin-18. Methods.
2 Arend W.P., Palmer G., Gabay C. (2008). IL-1, IL-18, and IL-33 families of cytokines. Immunol Rev.
3 Dinarello C.A. (2007). Interleukin-18 and the pathogenesis of inflammatory diseases. Semin Nephrol.
4 Dinarello C.A., Fantuzzi G. (2003). Interleukin-18 and host defense against infection. J Infect Dis.
5 Dinarello C.A. (2000). Targeting interleukin 18 with interleukin 18 binding protein. Ann Rheum Dis.
6 Faggioni R., Cattley R.C., Guo J., Flores S., Brown H., Qi M., Yin S., Hill D., Scully S., Chen C., Brankow D., Lewis J., Baikalov C., Yamane H., Meng T., Martin F., Hu S., Boone T., Senaldi G. (2001). IL-18-binding protein protects against lipopolysaccharide- induced lethality and prevents the development of Fas/Fas ligand-mediated models of liver disease in mice. J Immunol.
7 Dinarello C.A. (1996). Biologic basis for interleukin-1 in disease. Blood.
8 McColl B.W., Allan S.M., Rothwell N.J. (2009). Systemic infection, inflammation and acute ischemic stroke. Neuroscience.
9 Simi A., Tsakiri N., Wang P., Rothwell N.J. (2007). Interleukin-1 and inflammatory neurodegeneration. Biochem Soc Trans.
10 Dinarello C.A., Simon A., van der Meer J.W. (2012). Treating inflammation by blocking interleukin-1 in a broad spectrum of diseases. Nat Rev Drug Discov.
11 Neven B., Marvillet I., Terrada C., Ferster A., Boddaert N., Couloignier V., Pinto G., Pagnier A., Bodemer C., Bodaghi B., Tardieu M., Prieur A.M., Quartier P. (2010). Long-term efficacy of the interleukin-1 receptor antagonist anakinra in ten patients with neonatal-onset multisystem inflammatory disease/chronic infantile neurologic, cutaneous, articular syndrome. Arthritis Rheum.
12 Emsley H.C., Smith C.J., Georgiou R.F., Vail A., Hopkins S.J., Rothwell N.J., Tyrrell P.J. (2005). A randomised phase II study of interleukin-1 receptor antagonist in acute stroke patients. J Neurol Neurosurg Psychiatry.
13 Thompson R.C., Dripps D.J., Eisenberg S.P. (1992). Interleukin-1 receptor antagonist (IL-1ra) as a probe and as a treatment for IL-1 mediated disease. Int J Immunopharmacol.
14 Sims J.E. (2002). IL-1 and IL-18 receptors, and their extended family. Curr Opin Immunol.
15 Liu Z., Wyffels L., Barber C., Wan L., Xu H., Hui M.M., Furenlid L.R., Woolfenden J.M. (2012). Characterization of 99mTc-labeled cytokine ligands for inflammation imaging via TNF and IL-1 pathways. Nucl Med Biol.